# DiD-Labeled anti-EpCAM-directed NK-92-scFv(MOC31) zeta cells

Chemical name: | DiD-Labeled anti-EpCAM-directed NK-92-scFv(MOC31) zeta cells
Abbreviated name: | DiD-NK-92-scFv(MOC31) zeta cells
Synonym:
Agent category: | Antibody scFv fragment
Target: | Epithelial cell adhesion molecule (EpCAM)
Target category: | Adhesion molecule
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | 1,1’-Dioctadecyl-3,3,3’,3’-tetramethylindodicarbocyanine (DiD)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=218505670), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=218505669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4072) for more information about EpCAM.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals (4, 5).

Natural killer (NK) cells exert a high selective cytotoxicity against tumor cells without cytotoxicity against normal cells (6). Adoptive cancer immunotherapy has been performed with systemic infusion of ex vivo activated autologous or donor NK cells (7-9). Cellular immunotherapy with NK-92, a clonal NK cell line, has been initiated in a phase I clinical trial (http://www.clinicaltrials.gov/ct2/show/NCT00900809?term=NK-92+cellular+therapy&rank=1) against acute myeloid leukemia. The epithelial cell adhesion molecule (EpCAM) is found on the cell surface of epithelial cells of many epithelial tissues such as in the pancreas, jejunum, colon, kidney, salivary gland, and prostate (10). EpCAM is responsible for intracellular signaling and polarity, as well as mediation of cell differentiation, proliferation, migration, and adhesion (11, 12). EpCAM is a pan-epithelial (http://en.wikipedia.org/wiki/Epithelial) differentiation antigen (http://en.wikipedia.org/wiki/Antigen) that is expressed on almost all carcinomas (http://en.wikipedia.org/wiki/Carcinomas) (13). Approximately 70% of human prostate cancers show high levels of EpCAM expression (14, 15). Tavri et al. (16) have generated NK-92 cells transduced with a humanized single-chain Fv antibody fragment (scFv) of EpCAM antibody MOC31 fused with CD3 zeta chain and tagged with 1,1’-dioctadecyl-3,3,3’,3’-tetramethylindodicarbocyanine (DiD) (DiD-NK-92-scFv(MOC31) zeta cells) for noninvasive NIR imaging of EpCAM expression in prostate tumor cells in rats. DiD is a NIR fluorescence dye with an absorbance maximum at 644 nm and an emission maximum at 665 nm.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20rodentia)]

Tavri et al. (16) reported the labeling of NK-92-scFv(MOC31) zeta cells and NK-92 parental cells with DiD. The NK cells were incubated with 5 µg/ml DiD for 15 min and then washed three times with phosphate-buffered saline. The NK-92 parental cells showed one-fold higher labeling efficiency than the NK-92-scFv(MOC31) zeta cells. The labeling procedure had no effect on the NK cell viability.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20in%20vitro)]

NK-92-scFv(MOC31) zeta cells (not labeled with DiD) lysed EpCAM-expressing DU145 prostate cells, whereas the parental NK-92 showed no cell lysis (16). MOC31 monoclonal antibody blocked cytotoxicity by >90%. Fluorescence microscopy analysis showed that the dye was integrated into the cell membrane of labeled NK cells. The dye remained in the NK cells for up to 24 h after labeling.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20rodentia)]

Tavri et al. (16) performed whole-body NIR fluorescence imaging of rats (n = 6/group) bearing DU145 tumors after intravenous injection of 1.5 × 10^7^ DiD-NK-92-scFv(MOC31) zeta cells or 1.5 × 10^7^ DiD-NK-92 cells. There was an increase in fluorescence signal in the tumors at 1.5 and 8 h after injection of DiD-NK-92-scFv(MOC31) zeta cells, followed by a leveling off at 24 h. The fluorescence units were <1, 8, 12, and 11 at 0, 1.5, 8, and 24 h after injection, respectively. On the other hand, DiD-NK-92 parental cells showed <1 at all time points. Ex vivo NIR fluorescence imaging showed the tumor/liver, tumor/lung, tumor/spleen, and tumor/sternum ratios of 3, 5, 6, and 15 at 24 h after injection of DiD-NK-92-scFv(MOC31) zeta cells, respectively. In contrast, DiD-NK-92 parental cells exhibited tumor/nontargeted tissue ratios of <1. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NK-92-scFv%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Moretta L., Bottino C., Pende D., Vitale M., Mingari M.C., Moretta A. (2005). Human natural killer cells: Molecular mechanisms controlling NK cell activation and tumor cell lysis. Immunol Lett.
7 Klingemann H.G. (2005). Natural killer cell-based immunotherapeutic strategies. Cytotherapy.
8 Mercer J.C., Ragin M.J., August A. (2005). Natural killer T cells: rapid responders controlling immunity and disease. Int J Biochem Cell Biol.
9 Orange J.S., Ballas Z.K. (2006). Natural killer cells in human health and disease. Clin Immunol.
10 Trzpis M., McLaughlin P.M., de Leij L.M., Harmsen M.C. (2007). Epithelial cell adhesion molecule: more than a carcinoma marker and adhesion molecule. Am J Pathol.
11 Balzar M., Prins F.A., Bakker H.A., Fleuren G.J., Warnaar S.O., Litvinov S.V. (1999). The structural analysis of adhesions mediated by Ep-CAM. Exp Cell Res.
12 Balzar M., Winter M.J., de Boer C.J., Litvinov S.V. (1999). The biology of the 17-1A antigen (Ep-CAM). J Mol Med.
13 Armstrong A., Eck S.L. (2003). EpCAM: A new therapeutic target for an old cancer antigen. Cancer Biol Ther.
14 Poczatek R.B., Myers R.B., Manne U., Oelschlager D.K., Weiss H.L., Bostwick D.G., Grizzle W.E. (1999). Ep-Cam levels in prostatic adenocarcinoma and prostatic intraepithelial neoplasia. J Urol.
15 Went P.T., Lugli A., Meier S., Bundi M., Mirlacher M., Sauter G., Dirnhofer S. (2004). Frequent EpCam protein expression in human carcinomas. Hum Pathol.
16 Tavri S., Jha P., Meier R., Henning T.D., Muller T., Hostetter D., Knopp C., Johansson M., Reinhart V., Boddington S., Sista A., Wels W.S., Daldrup-Link H.E. (2009). Optical imaging of cellular immunotherapy against prostate cancer. Mol Imaging.